# 2-(2-(5-[^11^C]Methoxypyridin-3-yl)ethynyl)pyridine

Chemical name: | 2-(2-(5-[^11^C]Methoxypyridin-3-yl)ethynyl)pyridine
Abbreviated name: | [^11^C]M-PEPy
Synonym:
Agent Category: | Compound
Target: | Metabotropic glutamate subtype 5 (mGlu5) receptor (mGluR5 or mGluR_5_)
Target Category: | Receptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=metabotropic+glutamate+receptor+subtype+5+PET+ligand)]

2-(2-(5-[^11^C]Methoxypyridin-3-yl)ethynyl)pyridine ([^11^C]M-PEPy) is a radioligand developed for positron emission tomography (PET) imaging of metabotropic glutamate (mGlu) receptor subtype 5 (mGluR5 or mGluR_5_) in the central nervous system (CNS) (1, 2). ^11^C is a positron emitter with a physical half-life of 20.3 min.

Glutamate is a major excitatory neurotransmitter at CNS synapses. Many neuroanatomical CNS projection pathways contain glutamatergic neurons (3). Glutamate produces its excitatory effects by acting on cell-surface ionotropic glutamate or mGluRs (4). The mGluRs are G-protein–coupled receptors, and the eight mGluR subtypes are further subdivided into groups I, II, and III. The group I receptors include mGluR1 and mGluR5, and they are found predominantly in postsynaptic locations. The mGluR5s are found with high to moderate density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, hippocampus, and dorsal horn of the spinal cord, whereas the density in the cerebellum is low. These receptors couple with phospholipase C and up- or downregulate neuronal excitability. They have been implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal. These receptors are also involved in the modulation of various pain states, which makes them attractive targets for therapeutic drug development.

PET and single-photon emission computed tomography imaging of radioligands that target mGluR5s can be used to visualize and study the CNS mGluR5s in normal and pathological states. Some mGluR5 antagonists have been successfully labeled, but their in vivo visualization has been hampered by high lipophilicity, unfavorable brain uptake kinetics, or high metabolism (5, 6). 2-Methyl-6-(2-phenylethynylpyridine (MPEP) and its analogs, M-MPEP and M-PEPy, have been identified as potent and highly selective noncompetitive antagonists for mGluR5 (1, 7-9). M-MPEP was reported to have approximately six-fold higher in vitro affinity (50% inhibition concentration = 3.4 nM) compared to 5-[(2-methyl-1,3-thizaol-4-yl)-ethynyl]pyridine (MTEP), an mGluR5 antagonist with moderately high affinity (2, 9). Yu et al. (1) synthesized [^11^C]M-PEPy and demonstrated the feasibility of using it as a PET ligand for in vivo imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+synthesis)]

Cosford et al. (9) reported the synthesis of the phenolic precursor 5-(2-(pyridin-2-yl)ethynyl)pyridin-3-ol of M-PEPy. Briefly, sodium methoxide was reacted with 3,5-dibromopyridine in dimethylformamide at 60ºC for 18 h to produce 3-bromo-5-methoxypyridine. M-PEPy was prepared by Sonogoshira cross-coupling of 2-ethynylpyridine with 3-bromo-5-methoxypyridine. M-PEPy was converted to the phenolic precursor by reaction with methylene bromide in the presence of aluminum bromide at 0–25ºC for 1 h. The yield was 76%. Yu et al. (1) reported the radiosynthesis of [^11^C]M-PEPy by radiolabeling this phenolic precursor with [^11^C]methyl iodide ([^11^C]CH_3_I) under basic conditions. [^11^C]CH_3_I was prepared from [^11^C]carbon dioxide with the use of the ^14^N(p, α)^11^C reaction. The best yield condition was determined to be with the use of potassium hydroxide (KOH) as the base. In this radiolabeling reaction, 4–10 mg of solid KOH powder was added to 0.5–1.0 mg of the precursor dissolved in acetonitrile before [^11^C]CH_3_I was added to the reaction mixture. The mixture was heated at 90ºC for 6 min. The radioligand was purified with high-performance liquid chromatography (HPLC). The radiochemical purity was >98.1 ± 1.6% (n = 9), and the specific activity was 31 ± 4.4 GBq/μmol (840 ± 120 mCi/μmol). The radiochemical yield was 1.47 ± 0.70 GBq (39.8 ± 18.8 mCi) at the end of synthesis (EOS). The time of synthesis was ~45 min.

Severance et al. (2) reported the radiosynthesis of [^11^C]M-PEPy with the precursor desmethyl-M-PEPy with the use of [^11^C]methyl triflate, which was synthesized from [^11^C]methyl iodide. Desmethyl-M-PEPy was dissolved in acetone and mixed with aqueous sodium hydroxide. [^11^C]Methyl triflate was transported into the mixture at room temperature over a period of 5 min, and then mixture was heated at 60ºC for 2 min. The final product was purified with semipreparative HPLC; the radiochemical purity was >99%. The total time of synthesis was 30 min from the end of bombardment with an average yield of 30 ± 5.5% (n = 10) based on [^11^C]CO_2_ at EOS. The average specific activity of [^11^C]M-PEPy was 70.3 ± 33.3 GBq/μmol (1.9 ± 0.9 Ci/μmol) (n = 9).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+in+vitro)]

Severance et al. (2) studied the in vitro binding of [^11^C]M-MPEPy with the use of 20-μm sections of human prefrontal cortex, striatum, hippocampus, occipital cortex, and cerebellum, as well as rat brain sections. The sections were incubated with [^11^C]M-MPEP for 40 min. The sections were then washed and studied with a phosphor imager. Nonspecific binding was evaluated by coincubation with unlabeled M-MPEPy. High specific binding was observed in human brain sections of hippocampus, striatum, ventral striatum, frontal cortex, and occipital cortex. Similar high specific binding was also observed in the hippocampus and cortex of the rat brain sections. Minimal specific binding was found in the both human and rat cerebellum. The hippocampus/cerebellum ratio was ~8 in the human sections and ~37 in the rat sections.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+rodentia)]

Dynamic PET imaging of [^11^C]M-PEPy was performed in male rats (1). Each halothane-anesthetized rat received 111 ± 72.89 MBq (3.00 ± 1.97 mCi) [^11^C]M-PEPy in 0.43 ± 0.16 μg (2–3 nM in 0.1 ml or ~3.57 nmol calculated from the mean specific activity of 0.84 mCi/nmol) by i.v. administration. Dynamic imaging for 1 h after administration showed that the radioligand was primarily eliminated from the body through gastrointestinal pathways with accumulation of radioactivity in the liver, pancreas, and intestine. The radioactivity appeared to be in the bile and was excreted through the common bile duct. No accumulation of radioactivity was observed in the bladder during the 1 h of imaging. Imaging of the brain showed that the maximum radioactivity accumulation was in the olfactory area. The maximum value of the olfactory bulb/cerebellum radioactivity ratio was 8.1 at 10 min. At 10 min, the highest radioactivity level was in the olfactory bulb, followed by the striatum, hippocampus, and cortex. The authors suggested that this distribution pattern appeared to be similar to that of the brain mGluR5s in rats (10). The radioactivity levels (n = 13) of the whole brain in percentage of the injected dose per cubic centimeter (% ID/cc) as obtained from volumetric region-of-interest image analysis were 0.136 ± 0.097 (5 min), 0.099 ± 0.063 (10 min), 0.082 ± 0.051 (20 min), 0.074 ± 0.047 (30 min), 0.068 ± 0.044 (40 min), 0.061 ± 0.041 (50 min), and 0.050 ± 0.045 (60 min). The radioactivity levels (% ID/cc) of the olfactory bulb were 0.83 ± 0.79 (5 min), 0.73 ± 0.62 (10 min), 0.56 ± 0.42 (20 min), 0.45 ± 0.32 (30 min), 0.38 ± 0.26 (40 min), 0.36 ± 0.23 (50 min), and 0.30 ± 0.22 (60 min). The [^11^C]M-PEPy radioactivity levels were reversible in all areas of the body. When a blocking dose of 10 mg/kg unlabeled MPEP was administered intravenously 5 min before the radioligand injection (79.18 ± 56.98 MBq (2.96 ± 1.51 mCi) in 0.74 ± 0.38 μg (~3.52 nmol calculated from the mean specific activity of 0.84 mCi/nmol)), the radioactivity levels (n = 8) of the olfactory lobe were decreased by 84.6% at 5 min and by 60.5% at 40 min. In the other parts of the brain, MPEP decreased radioactivity levels of [^11^C]M-PEPy in the early time points: at 5 min the decreases were 44.9% in the whole brain, 47.3% in the striatum, 46.9% in the cortex, and 28.7% in the hippocampus; at 40 min, the corresponding decreases were 19.1% in the whole brain, 14.9% in the striatum, 28.1% in the cortex, and 31.4% in the hippocampus. No ex vivo verification was presented.

In the in vivo metabolism study, HPLC analysis showed [^11^C]M-PEPy to be rapidly metabolized after administration (1). The percentage of the radioligand that remained intact in the plasma after administration (n = 3) was 20.1 ± 4.9% at 10 min and 6.9 ± 3.1% at 30 min. No lipophilic metabolite from [^11^C]M-PEPy was found in the plasma.

Severance et al. (2) performed micro-PET imaging of [^11^C]M-PEPy in anesthetized (urethane) rats. Each rat received a dose of 12.53 ± 9.0 MBq (0.34 ± 0.24 mCi) [^11^C]M-PEPy with a specific activity of 61.94 ± 5.4 GBq/μmol (1.67 ± 0.15 Ci/μmol). Radioactivity was observed in the olfactory epithelium and the brain. The radioactivity reached a maximum at 2–3 min and then rapidly decreased. The average hippocampus/cerebellum ratio at 20 min was 1.6 ± 0.4. Ex vivo studies were conducted in rats without anesthesia (dose = 6.92 ± 2.66 MBq (0.19 ± 0.72 mCi); specific activity = 52.17 GBq/μmol (1.41 Ci/μmol)). The rats were euthanized after a 15-min brain imaging. The brains were removed, and different brain sections were dissected for counting. The average hippocampus/cerebellum radioactivity ratio was 1.8 ± 0.3.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+(primate+NOT+human))]

Yu et al. (1) briefly reported PET imaging studies of [^11^C]M-PEPy in primates. The authors observed that the basic radioactivity distribution was the same as that observed in rats; no data were presented. Severance et al. (2) performed two [^11^C]M-PEPy scans in one male baboon. A dose of 170.2 ± 16.3 MBq (4.6 ± 0.24 mCi) [^11^C]M-PEPy (specific activity = 119.88 ± 18.13 GBq/μmol (3.24 ± 0.49 Ci/μmol)) was administered to the baboon. Accumulation of radioactivity was observed throughout the brain. The highest radioactivity was found in the hippocampus and frontal cortex. The lowest radioactivity area was the cerebellum. The hippocampus/cerebellum and frontal cortex/cerebellum ratios of radioactivity at 20 min averaged 1.4 ± 0.1 and 1.2 ± 0.1, respectively; these ratios peaked between 10 and 20 min. The hippocampus/cerebellum ratio decreased to 1 by 40 min.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+human)]

No publication is currently available.

## NIH Support

NIH/NIBIB grant EB01850, PHS MH062185.

## References

1 Yu M., Tueckmantel W., Wang X., Zhu A., Kozikowski A.P., Brownell A.L. (2005). Methoxyphenylethynyl, methoxypyridylethynyl and phenylethynyl derivatives of pyridine: synthesis, radiolabeling and evaluation of new PET ligands for metabotropic glutamate subtype 5 receptors. Nucl Med Biol.
2 Severance A.J., Parsey R.V., Kumar J.S., Underwood M.D., Arango V., Majo V.J., Prabhakaran J., Simpson N.R., Van Heertum R.L., Mann J.J. (2006). In vitro and in vivo evaluation of [11C]MPEPy as a potential PET ligand for mGlu5 receptors. Nucl Med Biol.
3 Pin J.P., Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
4 Slassi A., Isaac M., Edwards L., Minidis A., Wensbo D., Mattsson J., Nilsson K., Raboisson P., McLeod D., Stormann T.M., Hammerland L.G., Johnson E. (2005). Recent advances in non-competitive mGlu5 receptor antagonists and their potential therapeutic applications. Curr Top Med Chem.
5 Ametamey S.M., Kessler L.J., Honer M., Wyss M.T., Buck A., Hintermann S., Auberson Y.P., Gasparini F., Schubiger P.A. (2006). Radiosynthesis and Preclinical Evaluation of 11C-ABP688 as a Probe for Imaging the Metabotropic Glutamate Receptor Subtype 5. J Nucl Med.
6 Patel S., Ndubizu O., Hamill T., Chaudhary A., Burns H.D., Hargreaves R., Gibson R.E. (2005). Screening cascade and development of potential Positron Emission Tomography radiotracers for mGluR5: in vitro and in vivo characterization. Mol Imaging Biol.
7 Gasparini F., Andres H., Flor P.J., Heinrich M., Inderbitzin W., Lingenhohl K., Muller H., Munk V.C., Omilusik K., Stierlin C., Stoehr N., Vranesic I., Kuhn R. (2002). [(3)H]-M-MPEP, a potent, subtype-selective radioligand for the metabotropic glutamate receptor subtype 5. Bioorg Med Chem Lett.
8 Patel S., Krause S.M., Hamill T., Chaudhary A., Burns D.H., Gibson R.A. (2003). In vitro characterization of [3H]MethoxyPyEP, an mGluR5 selective radioligand. Life Sci.
9 Cosford N.D., Roppe J., Tehrani L., Schweiger E.J., Seiders T.J., Chaudary A., Rao S., Varney M.A. (2003). [3H]-methoxymethyl-MTEP and [3H]-methoxy-PEPy: potent and selective radioligands for the metabotropic glutamate subtype 5 (mGlu5) receptor. Bioorg Med Chem Lett.
10 Shigemoto R., Nomura S., Ohishi H., Sugihara H., Nakanishi S., Mizuno N. (1993). Immunohistochemical localization of a metabotropic glutamate receptor, mGluR5, in the rat brain. Neurosci Lett.